# 4-[^18^F]Fluorobenzoyl-knottin 2.5D

Chemical name: | 4-[^18^F]Fluorobenzoyl-knottin 2.5D
Abbreviated name: | [^18^F]FB-2.5D
Synonym:
Agent Category: | Peptide
Target: | α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=knottin+peptides)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding (expressed as 50% inhibitory concentration (IC_50_)) to α_v_β_3_ (IC_50_, 7–40 nM) but not to α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM) integrins. Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). Only one cyclic RGD peptide used for imaging, [^18^F]fluoropropionyl-galacto-c(Arg-Gly-Asp-D-Phe-Lys) ([^18^F]-galacto-RGD), has been investigated for measuring expression of α_v_β_3_ integrin in cancer patients with tumors. However, [^18^F]-galacto-RGD has been shown to have low tumor accumulation and low signal/background ratios. Cystine knot peptides (knottins) share a common disulfide-bonded framework and a triple-stranded β-sheet fold (13). The integrin-binding RGD motif was grafted into a knottin from trypsin inhibitor II of the squash plant (Ecballium elaterium). Knottin 2.5D (with three disulfide bonds; (GCPQGRGDWAPTSCSQDSDCLAGCVCGPNGFCG-NH_2_) was identified from a series of genetically engineered knottin peptides to have nanomolar binding to the α_v_β_3_, α_v_β_5_, and α_5_β_1_ integrin receptors (14, 15). Knottin 2.5D was labeled with N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) to form 4-[^18^F]fluorobenzoyl-knottin 2.5D ([^18^F]FB-2.5D) and evaluated for positron emission tomography (PET) imaging of tumor xenografts in mice (16).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Knottin+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Knottin (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=841163)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=knot%20peptide)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+knottin+2%2E5D+synthesis)]

Knottin 2.5D was prepared with solid-phase peptide synthesis (16). The linear peptide was folded in the presence of 2.5 mM reduced glutathione and 20% dimethylsulfoxide (DMSO) in 0.1 M ammonium bicarbonate (pH, 9). Knottin 2.5D was purified with high-performance liquid chromatography. Peptide purity and molecular mass confirmed with MALDI-TOF mass spectroscopy and electrospray ionization mass spectrometery. To label with ^18^F, knottin 2.5D was incubated with ^18^F-SFB in DMSO for 1 h at 60°C. [^18^F]FB-2.5D was purified with HPLC. The total synthesis and purification time was 3 h with a radiochemical yield of 28% at the end of synthesis (EOS). The radiochemical purity and specific activity were >95% and ~100 GBq/µmol (2.7 Ci/µmol) at EOS, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+knottin+2%2E5D+in+vitro+studies)]

To determine the relative integrin-binding affinities (expressed as IC_50_ values) of 2.5D, FB-2.5D, and echistatin, a competition binding assay was performed with ^125^I-echistatin using U87MG human glioblastoma cells (16). The IC_50_ values for 2.5D, FB-2.5D, and echistatin were determined to be 20.3 ± 7.3, 13.2 ± 5.4, and 3.7 ± 1.1 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+knottin+2%2E5D+rodentia)]

Miao et al. (16) performed ex vivo biodistribution studies of [^18^F]FB-2.5D (0.74 MBq (20 μCi)) in nude mice (n = 3/group) bearing U87MG xenografts at 0.5 h after intravenous injection. The tracer accumulation in the tumors was 1.9 ± 1.2% injected dose per gram (ID/g). The organ with the highest radioactivity was the kidney (4.2 ± 0.2% ID/g), followed by the liver (1.4 ± 0.6% ID/g) and blood (1.3 ± 0.1% ID/g). The radioactivity in the bone was <0.5% ID/g. Co-administration of excess c(RGDyK) decreased tumor accumulation by 70% at 0.5 h after injection (P < 0.05), whereas little inhibition was observed in the kidneys, liver, and bone. PET analysis was performed in nude mice bearing U87MG tumors after intravenous injection of ~4.4 MBq (120 μCi) [^18^F]FB-2.5D. Tumors were clearly visualized at 0.5–1 h along with the kidneys, gall bladder, and urinary bladder. Tumor accumulation was determined to be 2.6% ID/g at 0.5 h and 1.5% ID/g at 1 h. Co-administration of excess c(RGDyK) decreased tumor accumulation by 75% at 0.5 h after injection (P < 0.05).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F+knottin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+knottin+2%2E5D+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+knottin+2%2E5D+Human+Studies)]

No references are currently available.

## NIH Support

5K 01 CA104706, 5R01 CA119053, R24 CA93862, P50 CA114747.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Pallaghy P.K., Nielsen K.J., Craik D.J., Norton R.S. (1994). A common structural motif incorporating a cystine knot and a triple-stranded beta-sheet in toxic and inhibitory polypeptides. Protein Sci.
14 Kimura R.H., Levin A.M., Cochran F.V., Cochran J.R. (2009). Engineered cystine knot peptides that bind alphavbeta3, alphavbeta5, and alpha5beta1 integrins with low-nanomolar affinity. Proteins.
15 Kimura R.H., Cheng Z., Gambhir S.S., Cochran J.R. (2009). Engineered knottin peptides: a new class of agents for imaging integrin expression in living subjects. Cancer Res.
16 Miao Z., Ren G., Liu H., Kimura R.H., Jiang L., Cochran J.R., Gambhir S.S., Cheng Z. (2009). An engineered knottin peptide labeled with 18F for PET imaging of integrin expression. Bioconjug Chem.